# [^11^C]N,N-Dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine

Chemical name: | [^11^C]N,N-Dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine
Abbreviated name: | [^11^C]HOMADAM
Synonym: | Carbon-11 HOMADAM
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

A number of neuropsychiatric disorders, including major depression, schizophrenia, and Alzheimer’s and Parkinson’s diseases (1-3), involve a dysfunction of the brain’s serotonin system. The serotonergic neurons – present in wide areas of the brain, including the hypothalamus, thalamus and cerebral cortex – bear a protein called “serotonin transporter” (SERT) (4).

SERT is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. It regulates neurotransmission by removing released serotonin from the extracellular space back into the presynaptic neuron. A variety of radioligands for positron emission tomography (PET) have been evaluated for imaging SERT. The most recent include [^11^C]N,N-dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB), [^11^C]2-(2-(dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine ([^11^C]AFM), [^11^C]5-bromo-2-[2-(dimethylaminomethylphenylthio)]phenylamine ([^11^C]DAPA), and [^11^C]2-[2-(dimethylaminomethylphenylthio)]-5-iodophenylamine ([^11^C]ADAM), which are PET radiotracers based on a diaryl sulfide motif (5).

A variety of in vivo radioligands for PET have been evaluated for imaging SERT. [^11^C]McN5652 was the first successful and widely used agent (6, 7) However, it does have some limitations related to its slow brain kinetics and low to nonspecific binding ratios in humans. [^11^C]McN5652 is adequate for regions with high SERT density but often provides insufficient signal-to-noise differentials for imaging brain regions with intermediate to low SERT densities (e.g., limbic and neocortical regions).

Over recent years, new PET radioligands have been synthesized and evaluated as SERT imaging agents and alternatives to [^11^C]McN5652. Among them, [^11^C]DASB, [^11^C]AFM, [^11^C]DAPA, and [^11^C]ADAM are based on a diaryl sulfide motif (4). [^11^C]N,N-Dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine ([^11^C]HOMADAM), a new benzylamine derivate, is a new PET radiotracer currently being investigated for its SERT imaging properties. It was synthesized as part of an effort to develop a radiotracer with both favorable SERT-specific binding properties and the ability to reach a quasi-equilibrium for SERT binding relatively shortly after injection.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

HOMADAM and its radiolabeling substrate, N-methyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamide, can be prepared by a multistep synthetic procedure described by Jarkas et al. (8). The first step involves coupling 2-bromo-5-acetoxymethyl-nitrobenzene with thiosalicylic acid to produce 2-(4´-acetoxymethyl-2´-nitrophenylthio)benzoic acid (58% yield reported by Jarkas et al. (8)), which is subsequently converted to the corresponding acid chloride by treatment with thionyl chloride and then reacted with methylamine and dimethylamine hydrochlorides. The resulting products, N-methyl-2-(4´-acetoxymethyl-2´-nitrophenylthio)benzamide and N,N-dimethyl-2-(4´-acetoxymethyl-2´-nitrophenylthio)benzamide, are obtained, with yields of 81% and 68%, respectively, reported by Jarkas et al. (8). Under catalytic hydrogenation, these products give the amines N-methyl-2-(4´-acetoxymethyl-2´-aminophenylthio)benzamide and N,N-dimethyl-2-(4´-acetoxymethyl-2´-aminophenylthio)benzamide (50% yield (8)). After reduction with BH_3_-tetrahydrofuran complex, HOMADAM and its radiolabeling substrate are obtained (yields of 35% and 47%, respectively, reported by Jarkas et al. (8)).

[^11^C]HOMADAM is obtained by reacting a solution of the radiolabeling substrate N-methyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamide (1.0 mg in 0.2 ml of dimethyl formamide at –20 °C) with [^11^C]CH_3_I (produced from [^11^C]CO_2_, as described by Plisson et al. (9)). The chemical and radiochemical purities obtained were >99%, and the overall yield was 25 ± 2% (9). The specific activity at the end of the procedure was approximately 28,490 MBq/µmol (770 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28in%20vitro%20OR%20cell%29)]

In vitro studies on murine and human embryonic kidney cells transfected with cDNAs for the human dopamine, serotonin, and norepinephrine transporters were performed by Jarkas et al. (8). They showed that HOMADAM competed for [^3^H]citalopram binding to SERT. The affinity of HOMADAM for [^3^H]citalopram binding in human embryonic kidney cells expressing SERT was 44 and 1.7 times lower than the affinities for ADAM and DASB, respectively. The authors reported an inhibition coefficient of HOMADAM for SERT of 0.6 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20primate)]

MicroPET brain imaging studies of male rhesus monkeys were performed by Jarkas et al. (8), for time periods ranging from 0 to 90 min after administration of [^11^C]HOMADAM (435 MBq/µmol (11.7 Ci/mmol)). Accumulation of the tracer was found in the midbrain, thalamus, pons, medulla, and occipital cortex, with a regional distribution consistent with binding to SERT-rich sites. The highest and lowest uptakes were found in the midbrain and the cerebellum, respectively. The maximum uptake of the tracer in the midbrain was obtained between ~13 and 22 min post injection, with a slow decrease thereafter (54%/h). In comparison, maximal binding for [^11^C]DASB in the midbrain was found at ~22-45 min post injection, with a decrease of 37%/h. The highest uptakes of [^11^C]HOMADAM in the thalamus and pons were found at ~9 and 12 min post injection.

In vivo displacement studies of [^11^C]HOMADAM, using R,S-citalopram, showed a rapid and very substantial reduction of radioactivity in the thalamus, midbrain, and other SERT-rich brain regions, reflecting the selective binding of [^11^C]HOMADAM to SERT. Displacement was also obtained by injection of R,S-reboxetine, a norepinephrine transporter-selective ligand with a high nanomolar affinity for SERT (8).

An arterial metabolite analysis performed by Jarkas et al. (8) showed one major polar metabolite (non-ether extractable) of [^11^C]HOMADAM. The abundance of this metabolite increased from 10% to 90% of the total plasma measured activity at 5 and 60 min post injection. Its identity was not pursued because of its improbable brain permeability. The remaining radioactivity appeared to be from nonmetabolized [^11^C]HOMADAM; no formation of lipophilic radiolabeled metabolites able to enter the brain was detected.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20human)]

No publication is currently available.

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 Huang Y, Hwang DR, Narendran R, Sudo Y, Chatterjee R, Bae SA, Mawlawi O, Kegeles LS, Wilson AA, Kung HF, Laruelle M. (2002). Comparative evaluation in nonhuman primates of five PET radiotracers for imaging the serotonin transporters: [11C]McN 5652, [11C]ADAM, [11C]DASB, [11C]DAPA, and [11C]AFM. J Cereb Blood Flow Metab.
6 Suehiro M, Scheffel U, Ravert HT, Dannals RF, Wagner HN. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
7 Ichimiya T, Suhara T, Sudo Y, Okubo Y, Nakayama K, Nankai M, Inoue M, Yasuno F, Takano A, Maeda J, Shibuya H. (2002). Serotonin transporter binding in patients with mood disorders: a PET study with [11C](+)McN5652. Biol Psychiatry.
8 Jarkas N, Votaw JR, Voll RJ, Williams L, Camp VM, Owens MJ, Purselle DC, Bremner JD, Kilts CD, Nemeroff CB, Goodman MM. (2005). Carbon-11 HOMADAM: a novel PET radiotracer for imaging serotonin transporters. Nucl Med Biol.
9 Plisson C, McConathy J, Martarello L, Malveaux EJ, Camp VM, Williams L, Votaw JR, Goodman MM. (2004). Synthesis, radiosynthesis, and biological evaluation of carbon-11 and iodine-123 labeled 2beta-carbomethoxy-3beta-[4'-((Z)-2-haloethenyl)phenyl]tropanes: candidate radioligands for in vivo imaging of the serotonin transporter. J Med Chem.